# N-{2-[4-(2-Methoxyphenyl)piperazinyl]ethyl}-N-(2-pyridyl)-N-(4-[^18^F]-fluoromethylcyclohexane)carboxamide

Chemical name: | N-{2-[4-(2-Methoxyphenyl)piperazinyl]ethyl}-N-(2-pyridyl)-N-(4-[^18^F]-fluoromethylcyclohexane)carboxamide
Abbreviated name: | [^18^F]MeFWAY
Synonym:
Agent category: | Compound
Target: | 5-HT_1A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiologic roles as a neurotransmitter in the central nervous system (1). It is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G protein-coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_ and 5-HT_1F_.

5-HT_1A_ receptors are abundantly present in the hippocampus, entorhinal cortex, frontal cortex, raphe nucleus and septum with the lowest densities are observed in the basal ganglia, substantia nigra and cerebellum (5). Some thalamic and hypothalamic nuclei have intermediate densities. 5-HT_1A_ receptors are involved in the mediation of emotion and the function of the hypothalamus. 5-HT_1A_ receptors are implicated in anxiety, depression, hallucinogenic behavior, motion sickness and eating disorders. Thus, there is a need for selective ligands to investigate the pharmacologic role of 5-HT_1A_ receptors.

There have been several studies to develop specific 5-HT_1A_ radioligands [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-HT1a%5BAll%20Fields%5D%20AND%20imaging%5BAll%20Fields%5D)], such as [carbonyl-^11^C]WAY 100635 (http://www.ncbi.nlm.nih.gov/books/NBK23263/), [^18^F]FPWAY (http://www.ncbi.nlm.nih.gov/books/NBK23137/) and [^18^F]MPPF (http://www.ncbi.nlm.nih.gov/books/NBK23391/), for positron emission tomography imaging. However, some of these compounds lack good resistance to in vivo metabolism (6) or exhibit substantial cleavage of the ^18^F-fluorine bond (7), causing difficulties in using the reference region method for determination of brain 5-HT_1A_ receptor densities . N-{2-[4-(2-Methoxyphenyl)piperazinyl]ethyl}-N-(2-pyridyl)-N-(4-fluoromethylcyclohexane)carboxamide (MeFWAY), a fluoromethyl derivative to the cyclohexyl-ring of WAY-100635, was reported to be a potent inhibitor of 5-HT_1A_ receptors and to provide more resistance towards defluorination and metabolism in vivo. This led to the development of N-{2-[4-(2-methoxyphenyl)piperazinyl]ethyl}-N-(2-pyridyl)-N-(4-[^18^F]-fluoromethylcyclohexane)carboxamide ([^18^F]MeFWAY) as a useful tool for 5-HT_1A_ receptor positron emission tomography (PET) imaging in vivo (8).

### Related Resource Links:

- Chapters in MICAD (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT1A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/gene/3350))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_1A_ (http://www.ncbi.nlm.nih.gov/omim/109760))
- Clinical trials (5-HT_1A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT1A))
- Drug information in Food and Drug Administration (5-HT_1A_ (http://google2.fda.gov/search?q=5-HT1a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20synthesis)]

The reported radiosynthesis of [^18^F]MeFWAY by Saigal et al. (8) involved standard ^18^F-nucleophilic fluorination of the corresponding tosylate precursor, N-{2-[4-(2-methoxyphenyl)piperazinyl]ethyl}-N-(2-pyridyl)-N-(4-tosyloxymethylcyclohexane)carboxamide, with K[^18^F]F/Kryptofix2.2.2 in acetonitrile at 96°C for 30 min in an automated radiosynthesis unit, followed by high-performance liquid chromatography purification. The reported overall radiochemical yield of the radiosynthesis was 10-20% at the end of synthesis, the specific radioactivity was 74-111 GBq/µmol (2-3 Ci/µmol), and the radiochemical purity was >95%. Lipophilicity (log P) of [^18^F]MeFWAY was found to be 2.62 ± 0.06.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20in%20vitro)]

In vitro autoradiography studies of rat brain slices indicated the highest binding of [^18^F]MeFWAY to the hippocampus, colliculus, cortex and the lowest in the cerebellum, consistent with 5-HT_1A_ receptor distribution (8). The hippocampus/cerebellum, colliculus/cerebellum, and cortex/cerebellum ratios were 82, 46, and 40, respectively. Serotonin inhibited [^18^F]MeFWAY binding with IC_50_ values of 169 ± 5, 218 ± 15, and 244 ± 2 nM for the hippocampus, cortex, and colliculus, respectively. MeFWAY and WAY-100635 inhibited [^18^F]MeFWAY binding to the brain regions with IC_50_ values of 25.7 ± 2.4 and 23.2 ± 2.8 nM for the hippocampus, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20rodentia)]

Choi et al. (9) performed dynamic PET imaging studies for 120 min in rats after intravenous injection of 15-20 MBq (0.41-0.54 mCi) [^18^F]MeFWAY. Baseline tissue time-activity curves revealed a high accumulation of radioactivity that peaked at 5 min in the hippocampus, frontal cortex and cerebellum. However, the washout pattern was the slowest in the hippocampus, followed by the frontal cortex and cerebellum. Standard uptake values (SUVs) at 75 min were 6.41, 1.25, 0.95, and 0.4 for the skull, hippocampus, frontal cortex, and cerebellum, respectively. Binding potential (BP_ND_) values for the hippocampus and frontal cortex were 5.5 and 2.7 at 75 min using the cerebellum as a reference, respectively. Pretreatment with fluconazole (an inhibitor of MeFWAY metabolism in rat live microsomes, 60 mg/kg, 60 min) reduced the SUV in the skull (1.1) but increased the SUVs in the hippocampus (3.2) and frontal cortex (1.8) with little change in the cerebellum (0.5) at 75 min. Pretreatment with WAY-100635 reduced the radioactivity in the brain by 88% at 20 min. Displacement studies were performed at 30 min after tracer injection. WAY-100635 produced a rapid decrease in radioactivity in the brain with 66% inhibition at 120 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20nonhuman%20primate)]

The brain accumulation of radioactivity was studied by PET imaging in a rhesus monkey after intravenous injection of 130 MBq (3.5 mCi) of [^18^F]MeFWAY, with a rapid accumulation in the various brain regions of >0.03%ID/ml in <2 min (8). [^18^F]Mefway images (up to 180 min after injection) displayed radioactivity concentrations that followed a rank order: the hippocampus and insular cortex (tissue/cerebellum ratios of 8 to 10) > temporal cortex, cingulate gyrus, frontal cortex, and occipital cortex (tissue/cerebellum ratios of 5 to 8) > striatum, thalamus, and raphe (tissue/cerebellum ratios of 2 to 3.5) > cerebellum. The tissue/cerebellum ratios peaked at ~80 min with gradual decreases thereafter. The hippocampus/cerebellum ratio is similar to that of [carbonyl-^11^C]WAY 100635 (10) and better than that of [^18^F]MPPF (11). After injection of [^18^F]MeFWAY in the monkey, 40-50% and 30% of the total plasma radioactivity was intact [^18^F]MeFWAY at 50 and 180 min, respectively. There was one hydrophilic metabolite representing the amide-hydrolysis product, 4-[^18^F]fluoromethylcyclohexane carboxylic acid. Little radioactivity was detected in the skull of the monkey, indicating that there was little defluorination of [^18^F]MeFWAY. No blocking experiment was performed.

Wooten et al. (12) compared dynamic PET brain imaging studies of [^18^F]MeFWAY, [^18^F]MPPF, and [^11^C]WAY100635 in four rhesus monkeys for 120 min. High 5-HT_1A_ radioactivity levels were observed in the anterior cingulate cortex (ACG), mesial temporal cortex (MTC), raphe nuclei (RN) and insula cortex (IC). The BP_ND_ in the brain regions were; MTC: 7.4 ± 0.6, 3.1 ± 0.4, 7.0 ± 1.2, ACG: 7.2 ± 1.2, 2.1 ± 0.2, 7.9 ± 1.2; RN: 3.7 ± 0.6, 1.3 ± 0.3, 3.3 ± 0.7 and IC: 4.2 ± 0.6, 1.2 ± 0.1, 4.7 ± 1.0 for [^18^F]MeFWAY, [^18^F]MPPF, and [^11^C]WAY100635, respectively. These data indicate that [^18^F]MeFWAY and [^11^C]WAY100635 have very similar in vivo kinetics throughout the regions of the brain and provides the BP_ND_ values of 1-2 folds higher than [^18^F]MPPF in the rhesus monkey.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Mefway%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
3 Charney D.S. (1998). Monoamine dysfunction and the pathophysiology and treatment of depression. J Clin Psychiatry.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Pazos A., Probst A., Palacios J.M. (1987). Serotonin receptors in the human brain--III. Autoradiographic mapping of serotonin-1 receptors. Neuroscience.
6 Slifstein M., Parsey R.V., Laruelle M. (2000). Derivation of [(11)C]WAY-100635 binding parameters with reference tissue models: effect of violations of model assumptions. Nucl Med Biol.
7 Carson R.E., Wu Y., Lang L., Ma Y., Der M.G., Herscovitch P., Eckelman W.C. (2003). Brain uptake of the acid metabolites of F-18-labeled WAY 100635 analogs. J Cereb Blood Flow Metab.
8 Saigal N., Pichika R., Easwaramoorthy B., Collins D., Christian B.T., Shi B., Narayanan T.K., Potkin S.G., Mukherjee J. (2006). Synthesis and biologic evaluation of a novel serotonin 5-HT1A receptor radioligand, 18F-labeled MeFWAY, in rodents and imaging by PET in a nonhuman primate. J Nucl Med.
9 Choi J.Y., Kim C.H., Jeon T.J., Kim B.S., Yi C.H., Woo K.S., Seo Y.B., Han S.J., Kim K.M., Yi D.I., Lee M., Kim D.G., Kim J.Y., Lee K.C., Choi T.H., An G., Ryu Y.H. (2012). Effective microPET imaging of brain 5-HT(1A) receptors in rats with [(18) F]MeFWAY by suppression of radioligand defluorination. Synapse.
10 Osman S., Lundkvist C., Pike V.W., Halldin C., McCarron J.A., Swahn C.G., Farde L., Ginovart N., Luthra S.K., Gunn R.N., Bench C.J., Sargent P.A., Grasby P.M. (1998). Characterisation of the appearance of radioactive metabolites in monkey and human plasma from the 5-HT1A receptor radioligand, [carbonyl-11C]WAY-100635--explanation of high signal contrast in PET and an aid to biomathematical modelling. Nucl Med Biol.
11 Shiue C.Y., Shiue G.G., Mozley P.D., Kung M.P., Zhuang Z.P., Kim H.J., Kung H.F. (1997). P-[18F]-MPPF: a potential radioligand for PET studies of 5-HT1A receptors in humans. Synapse.
12 Wooten D.W., Moraino J.D., Hillmer A.T., Engle J.W., Dejesus O.J., Murali D., Barnhart T.E., Nickles R.J., Davidson R.J., Schneider M.L., Mukherjee J., Christian B.T. (2011). In vivo kinetics of [F-18]MEFWAY: a comparison with [C-11]WAY100635 and [F-18]MPPF in the nonhuman primate. Synapse.